# 3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_

Chemical name: | 3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_
Abbreviated name: | [^18^F]BAY 86-4367
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids), which binds to the GRP receptor (GRPR) with high affinity and specificity (1). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (2). Specific BBN receptors have been identified on CNS and GI tissues, including the pancreas, as well as on a number of tumor cell lines. The BBN-receptor superfamily includes at least four different subtypes: neuromedin B (NMB or BB1), the GRPR subtype (BB2), the BB3 subtype, and the BB4 subtype (3). The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR.

Currently used targeting GRPR peptides are primarily agonists. Therefore, there is a need for GRPR antagonist radioligands because antagonists usually bind to both high and low affinity sites of the target receptor and agonists only bind to high affinity sites. Llinares et al. (4) developed a series of GRPR peptide antagonists. One of them, D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM26), has been found to be a selective GRPR antagonist. A DOTA-Gly-benzoyl group was added to the C-terminus to form DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM1). For evaluation as a single-photon emission computed tomography imaging agent for GRPR, RM1 has been labeled with ^111^In to form ^111^In-RM1 (http://www.ncbi.nlm.nih.gov/books/NBK23333/) (5). A new GRPR peptide antagonist, DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM2), has been found to have a higher affinity for GRPR than RM1 and has been labeled with ^68^Ga for positron emission tomography (PET) imaging (6). 3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_ ([^18^F]7b (http://www.ncbi.nlm.nih.gov/books/NBK51677/)) was reported to have high prostate tumor accumulation (7). To increase the hydrophilicity of this agent, Honer et al. (8) inserted one more Ala(SO_3_H) moiety in the linker of [^18^F]7b to form 3-cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_ ([^18^F]BAY 86-4367). [^18^F]BAY 86-4367 showed specific and effective tumor targeting in prostate cancer xenografts in nude mice.

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GRPR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925))
- Articles in OMIM (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=Gastrin-releasing+peptide+receptor+))
- Drug information in FDA (GRPR (http://google-test.fda.gov/search?q=GASTRIN-RELEASING+PEPTIDE+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+synthesis)]

Honer et al. (8) prepared [^18^F]BAY 86-4367 with a one-step radiosynthesis. The precursor peptide, 3-cyano-4-trimethylammonium-benzoyl-Ala(SO_3_H)-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_, was prepared by solid-phase peptide synthesis. [^18^F]BAY 86-4367 was synthesized using a standard aromatic nucleophilic substitution ([^18^F]KF/Kryptofix 2.2.2) reaction (90°C, 10 min), with 15% decay-corrected yield and >95% radiochemical purity. The specific activity of [^18^F]BAY 86-4367 was 170 GBq/µmol (4.6 Ci/µmol) at the end of synthesis. The total synthesis time was not reported. [^18^F]BAY 86-4367 was stable in mouse and human plasma at 37°C for up to 120 min. [^nat^F]BAY 86-4367 exhibited a log D_7.4_ of −3.9.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+in+vitro)]

Honer et al. (8) performed in vitro saturation binding studies using GRPR-rich PC-3 human prostate cells (~50,000 binding sites/cell) with [^18^F]BAY 86-4367. There was a single high-affinity binding site with a dissociation constant of 1.43 ± 0.25 nM (n = 3). Inhibition binding studies of unlabeled BAY 86-4367 with ^125^I-BBN showed a 50% inhibition concentration (IC_50_) value of 0.94 ± 0.19 nM (n = 3). Unlabeled BAY 86-4367 inhibited the calcium release and receptor internalization induced by BBN, thereby suggesting antagonist behavior.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+rodentia)]

Honer et al. (8) performed ex vivo biodistribution studies with ~0.24 MBq (6.5 μCi) [^18^F]BAY 86-4367 in nude mice (n = 3/group) bearing PC-3 tumors. Tumor accumulation values, presented as % injected dose per gram (ID/g), for [^18^F]BAY 86-4367 were 4.6 ± 0.2% ID/g, 5.0 ± 1.2% ID/g, 5.9 ± 1.1% ID/g, and 6.2 ± 2.5% ID/g at 10, 20, 30, and 160 min after injection, respectively. [^18^F]BAY 86-4367 exhibited fast blood clearance, with 0.3% ID/g at 60 min after injection. The tumor/blood ratios were 2.5, 7.0, 8.9, and 18.6 at 10, 20, 30, and 160 min after injection, respectively. Accumulation in the GRPR-rich pancreas was 36% ID/g at 60 min after injection. The initial accumulation was moderate in the kidney, liver, adrenal gland, stomach, and intestine at 10 min after injection, with rapid washout by 60 min. Accumulation in the gallbladder was high, with 30%–50% ID/g at these time points, indicating rapid liver metabolism. The accumulation was low in other tissues, including bone. At 60 min, >50% ID of radioactivity was detected in the urine. There was only one minor polar radiometabolite (~15%) in the plasma at 15 min after injection, whereas there was one prominent hydrophilic radiometabolite (~85%) and two minor polar radiometabolites in the urine at 15 min after injection. Accumulation in the tumor and pancreas was effectively blocked (reduced by >80%) by co-administration of excess BBN. Some specific blocking was also observed in the adrenal gland, stomach, and intestine. [^18^F]BAY 86-4367 showed higher tumor accumulation (6.2 ± 2.5% ID/g) in the PC-3 tumor model at 60 min after injection than [^18^F]FDG (2.4 ± 0.2% ID/g) and [^18^F]choline (1.0 ± 0.1% ID/g) at the same time point.

PET imaging in nude mice (n = 2) bearing PC-3 xenografts was performed with 9–20 MBq (0.24–0.54 mCi) [^18^F]BAY 86-4367 60–105 min after injection (8). The tumors, intestine, gallbladder, and urinary bladder were clearly visualized. The pancreas was not clearly visualized because of the proximity to the bowel. Coinjection of excess BBN peptide inhibited the visualization of the tumor. Postmortem tissue sampling of these mice after PET scanning (107 min after injection) showed that the PET imaging data were similar to those obtained in the ex vivo biodistribution studies. The radioactivity levels in the GRPR-rich tumor and pancreas were 4.7% ID/g and 15.6% ID/g, respectively. The specificity of accumulation amounted to 82% and 96% for the tumor and pancreas, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAY%2086-4367+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
3 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
4 Llinares M., Devin C., Chaloin O., Azay J., Noel-Artis A.M., Bernad N., Fehrentz J.A., Martinez J. (1999). Syntheses and biological activities of potent bombesin receptor antagonists. J Pept Res.
5 Mansi R., Wang X., Forrer F., Kneifel S., Tamma M.L., Waser B., Cescato R., Reubi J.C., Maecke H.R. (2009). Evaluation of a 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated bombesin-based radioantagonist for the labeling with single-photon emission computed tomography, positron emission tomography, and therapeutic radionuclides. Clin Cancer Res.
6 Mansi R., Wang X., Forrer F., Waser B., Cescato R., Graham K., Borkowski S., Reubi J.C., Maecke H.R. (2011). Development of a potent DOTA-conjugated bombesin antagonist for targeting GRPr-positive tumours. Eur J Nucl Med Mol Imaging.
7 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
8 Honer M., Mu L., Stellfeld T., Graham K., Martic M., Fischer C.R., Lehmann L., Schubiger P.A., Ametamey S.M., Dinkelborg L., Srinivasan A., Borkowski S. (2011). 18F-labeled bombesin analog for specific and effective targeting of prostate tumors expressing gastrin-releasing peptide receptors. J Nucl Med.